# [^11^C]N-(3-Ethynylphenyl)-6,7-bis(2-methoxyethoxy)-4-quinazolinamine

Chemical name: | [^11^C]N-(3-Ethynylphenyl)-6,7-bis(2-methoxyethoxy)-4-quinazolinamine
Abbreviated name: | [^11^C]Erlotinib
Synonym: | [^11^C]Tarceva® or [^11^C]OSI-774
Agent Category: | Compound
Target: | Tyrosine kinase
Target Category: | Enzyme
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information on [^11^C]Erlotinib in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C+Erlotinib)]

Erlotinib is a selective tyrosine kinase (TK) inhibitor. The ^11^C-labeled form of erlotinib ([^11^C]erlotinib) was developed as a positron emission tomography (PET) tracer to identify erlotinib-sensitive tumors by evaluating epidermal growth factor receptor (EGFR) expression (1).

The EGF family of TK receptors consists of four members: EGFR, ErbB2, ErbB3, and ErbB4 (2). EGFR is also sometimes referred to as ErbB1 or Her1 Binding of the ligands to the extracellular domain of EGFR results in activation of the receptor by forming an active homodimer or heterodimer with the other EGFR members. As a result, several tyrosine residues in the C-terminal domain of EGFR are autophosphorylated, and its intracellular tyrosine kinase is activated. Upon activation, several important signal transduction cascades, including mitogen-activated protein kinase, Akt, and c-Jun N-terminal kinase pathways, are initiated and lead to DNA synthesis and cell proliferation. Overexpression of EGFR is a hallmark of several types of cancers, such as lung, brain, breast, pancreas, and head and neck cancers (2, 3). A specific mutation of EGFR, called EGFRvIII, is frequently detected in non-small cell lung cancer (NSCLC) and glioblastoma multiforme (3, 4). Because of its overexpression and oncogenic role in the development and progression of cancer, EGFR has attracted much attention for developing EGFR-targeted therapeutic and imaging agents (5).

Erlotinib and gefitinib (ZD1839) are the two most commonly used TK inhibitors that target the EGFR TK. Both compounds bind to the adenosine triphosphate–binding site of the enzyme and inhibit phosphorylation of the tyrosine residues. Erlotinib and gefitinib are approved by the United States Food and Drug Administration (FDA) for the treatment of NSCLC (3, 6) and are being evaluated in clinical trials (erlotinib (http://clinicaltrials.gov/ct2/results?term=Erlotinib), gefitinib (http://clinicaltrials.gov/ct2/results?term=gefitinib)) for other cancers. Erlotinib is also approved by the FDA to treat pancreatic cancer (http://www.cancer.gov/cancertopics/druginfo/fda-erlotinib-hydrochloride). The overall tumor response rate for erlotinib and gefitinib treatment was reported to be only 10–15% for NSCLC patients. However, erlotinib has been shown to have a survival benefit for patients with advanced NSCLC who have failed all prior treatment regimens (3, 6).

The low rate of tumor response to TK inhibitor treatment has led to the development of noninvasive methods that can be used to identify patients who are most likely to benefit from the treatment. Expression and mutation status of the EGFR in tumors is one of the most valuable parameters to help predict tumor response (7). However, this analysis usually requires a tumor biopsy, which may not be available in all cases. To noninvasively image EGFR expression, several groups have independently developed strategies to label gefitinib with ^18^F or ^11^C and tested their feasibility as PET tracers (8-11). Unfortunately, these studies indicate that radiolabeled gefitinib does not show EGFR-specific accumulation in human tumor xenografts because of its nonspecific binding. Radiolabeled gefitinib, however, may be used for the noninvasive study of the tissue pharmacokinetics and intratumoral drug concentrations of gefitinib (8-11). As an alternative, Memon et al. labeled erlotinib with ^11^C ([^11^C]erlotinib) and evaluated its use as a potential radiotracer for the identification of tumors in mice carrying either sensitive or less sensitive xenografts (1). The studies have shown that PET imaging with [^11^C]erlotinib can be used to identify erlotinib-sensitive lung cancer xenografts in mice.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C+Erlotinib%20AND%20synthesis)]

Memon et al. synthesized [^11^C]erlotinib by reacting 6-O-desmethyl-erlotinib with [^11^C]methyl iodide (1). The reaction was carried out in dimethyl formamide for 5 min at 120ºC, using sodium hydride as the supporting base. The reaction mixture was purified using high-performance liquid chromatography, evaporated at 100ºC under vacuum, and reformulated in a sterile saline and ethanol mixture (9:1). The specific activity of the labeled erlotinib was reported to be 20–100 GBq/µmol (0.54–2.7 Ci/µmol). The detailed radiochemical purity and stability of the agents were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20Erlotinib%20AND%20in%20vitro)]

Memon et al. analyzed the sensitivity of tumor cells to erlotinib treatment under in vitro conditions (1). Three lung cancer cell lines (HCC827, A549, and NCI358) and in vitro cell proliferation assays were used to determine the sensitivity after treatment with 0.5–6 µmol/L erlotinib for 48 hours. A significant dose-dependent inhibition of HCC827 cell proliferation was observed with erlotinib treatment. In contrast, A549 and NCI358 cells were less sensitive to erlotinib treatment as concentrations of erlotinib up to 6 µmol/L did not result in a significant decrease in proliferation. HCC827 cells are known to express high levels of EGFR and also harbor an in-frame deletion mutation (delE746-A750) in exon 19. A549 and HCC827 have been previously characterized as less sensitive and sensitive, respectively, to treatment with gefitinib (12). Memon et al. further confirmed with Western blot analysis that HCC827 cells expressed a higher level of active (phosphorylated) and total EGFR than either A549 or NCI358 cells (1).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C+Erlotinib%20AND%20rodentia)]

Biodistribution of [^11^C]erlotinib was analyzed in animal models of human lung cancer xenografts (1). The xenografts were produced with subcutaneous inoculation of tumor cells from each cell line (HCC827, A549, and NCI358) in the left shoulder of female BALB/cA nude mice (~8 weeks old). Tumor xenografts at ~1 cm in diameter were used in these studies. [^11^C]Erlotinib (15–20 MBq (0.41–0.54 mCi)) was injected as a bolus through the tail vein of each animal in the three models (A549, n = 3 mice; NCI358, n = 3 mice; HCC827, n = 2 mice). The major organs, tumors, and blood were collected 1 h after injection, and the accumulated [^11^C]erlotinib radioactivity in each organ was measured. In all xenograft models, the liver showed the highest amount of [^11^C]erlotinib (14.94, 13.34, and 10.55% injected dose per gram (ID/g) for A549, NCI358, and HCC827, respectively). Little to no activity was detected in the brain. The radioactivity in the blood was dependent on the animal models (1.06, 0.56, and 0.53% ID/g for A549, NCI358, and HCC827, respectively). HCC827 tumor xenografts showed a significantly higher accumulation (P < 0.05) of [^11^C]erlotinib (3.66 ± 0.14% ID/g) than A549 (1.62 ± 0.47% ID/g) and NCI358 (0.69 ± 0.11% ID/g). There was no significant difference (P > 0.05) between A549 and NCI358 for the accumulation of activity. No blocking studies were reported.

Dynamic micro-PET imaging of lung cancer xenografts was performed for 90 min after injection of 10–15 MBq (0.27–0.41 mCi) [^11^C]erlotinib via the tail vein (1). As expected, tumor xenografts from the erlotinib-sensitive HCC827 cells could be clearly detected with PET scanning. A high level of uptake was seen in HCC827 xenografts, whereas no significant uptake was observed in the A549 and NCI358 xenografts. The time–activity curves revealed a higher signal in tumors than in reference areas in the HCC827 xenografts, but not in the A549 and NCI358 xenografts, throughout the measurement period of 90 min. The activity was also sustained for a longer time in the HCC827 tumors than in the A549 and NCI358 tumors. The results suggest that PET imaging with [^11^C]erlotinib can be used as a noninvasive and rapid method for the identification of erlotinib-sensitive tumors in mice. No blocking experiment was performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Memon A.A., Jakobsen S., Dagnaes-Hansen F., Sorensen B.S., Keiding S., Nexo E. (2009). Positron emission tomography (PET) imaging with [11C]-labeled erlotinib: a micro-PET study on mice with lung tumor xenografts. Cancer Res.
2 Sorkin A., Goh L.K. (2008). Endocytosis and intracellular trafficking of ErbBs. Exp Cell Res.
3 Harari P.M., Allen G.W., Bonner J.A. (2007). Biology of interactions: antiepidermal growth factor receptor agents. J Clin Oncol.
4 Irmer D., Funk J.O., Blaukat A. (2007). EGFR kinase domain mutations - functional impact and relevance for lung cancer therapy. Oncogene.
5 Gelovani J.G. (2008). Molecular imaging of epidermal growth factor receptor expression-activity at the kinase level in tumors with positron emission tomography. Cancer Metastasis Rev.
6 Bareschino M.A., Schettino C., Troiani T., Martinelli E., Morgillo F., Ciardiello F. (2007). Erlotinib in cancer treatment. Ann Oncol.
7 Chen C.M., Chang J.W., Cheung Y.C., Lin G., Hsieh J.J., Hsu T., Huang S.F. (2008). Computed tomography-guided core-needle biopsy specimens demonstrate epidermal growth factor receptor mutations in patients with non-small-cell lung cancer. Acta Radiol.
8 Su H., Seimbille Y., Ferl G.Z., Bodenstein C., Fueger B., Kim K.J., Hsu Y.T., Dubinett S.M., Phelps M.E., Czernin J., Weber W.A. (2008). Evaluation of [(18)F]gefitinib as a molecular imaging probe for the assessment of the epidermal growth factor receptor status in malignant tumors. Eur J Nucl Med Mol Imaging.
9 Wang J.Q., Gao M., Miller K.D., Sledge G.W., Zheng Q.H. (2006). Synthesis of [ ^ 11 ^ C]Iressa as a new potential PET cancer imaging agent for epidermal growth factor receptor tyrosine kinase. Bioorg Med Chem Lett.
10 Seimbille Y. (2005). P.M.E., Czernin J., Silverman D.S., Fluorin-18 labeling of 6,7-distributed anilinoquinazoline derivatives, for positron emission tomography (PET) imaging of tyrosine kianse receptors:synthesis of 18F-Iressa and related molecular probes. J Labelled Compd Radiopharm.
11 Holt D.P. (2006). R.H.T., Dannals R.F., Pomper M.G., Pomper M.G. Synthesis of [^11^C]gefitinib for imaging epidermal growth factor receptor tyrosine kinase with positron emission tomography. J Labelled Compd Radiopharm.
12 Mukohara T., Engelman J.A., Hanna N.H., Yeap B.Y., Kobayashi S., Lindeman N., Halmos B., Pearlberg J., Tsuchihashi Z., Cantley L.C., Tenen D.G., Johnson B.E., Janne P.A. (2005). Differential effects of gefitinib and cetuximab on non-small-cell lung cancers bearing epidermal growth factor receptor mutations. J Natl Cancer Inst.